# OG488-Cyclo(Cys-Asn-Gly-Arg-Cys)-Gly-Lys

Chemical name: | OG488-Cyclo(Cys-Asn-Gly-Arg-Cys)-Gly-Lys
Abbreviated name: | OG488-cNGR
Synonym:
Agent category: | Peptide
Target: | Aminopeptidase N (CD13)
Target category: | Enzyme
Method of detection: | Optical, fluorescence imaging
Source of signal/contrast: | OG488
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Fibrosis is the formation of excess fibrous connective tissue (mainly collagen type I) in an organ or tissue as a reparative or reactive process in many chronic diseases in the heart, liver, kidneys, lungs, or vasculature.

Tumor angiogenesis represents a continuous and important process in tumor development in which the tumor attempts to gain an independent blood supply (3). This process is driven by the tumor's overproduction of angiogenic factors, which bind to receptors on nearby vessel endothelial cells. Angiogenesis is essential for the growth of solid tumors and their metastases. Imaging angiogenesis may be useful for monitoring angiogenic treatments of tumors and cardiovascular diseases (4-6). Aminopeptidase N (APN, CD13) is a membrane bound glycoprotein with MMP activity that cleaves unsubstituted, N-terminal amino acids with neutral side chains from peptides (7). APN has been shown to play a role in tumor angiogenesis, invasion, and metastasis (8). In addition to endothelial cells of angiogenic vessels, most cells of myeloid origin, epithelial cells, fibroblasts and smooth muscle cells also express CD13 (9, 10). The tumor homing peptide cyclo(Cys-Asn-Gly-Arg-Cys)-Gly-Lys (cNGR) contains the Asn-Gly-Arg (NGR) motif that binds to APN (11). Buehler et al. (12) has conjugated cNGR with Oregon Green 488 (OG488) to study angiogenesis in a murine myocardial infarction model.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EP-3533+synthesis)]

Cyclic NAc-Cys-Asn-Gly-Arg-Cys-Gly-Gly-Lys(Ac)-NH_2_ peptide was synthesized using solid-phase peptide synthesis and then labeled on the resin with Oregon Green 488 (OG488) via the ε-amino group of the lysine (12). OG488-cNGR was purified with high-pressure liquid chromatography with >95% purity. The molar ratio of Cy5.5 to cNGR was estimated to be ~1.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+in+vitro)]

Histoimmunostaining of CD13 was performed on HT-1080 and MCF-7 cancer cell lines (13). The APN enzyme was expressed in HT-1080 tumor cells, whereas expression in MCF-7 tumor cells was near background level. The APN activity in HT-1080 cells could be blocked with anti-CD13 antibodies and the cNGR peptide.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EP-3533+rodentia)]

Buehler et al. (12) studied OG488-cNGR homing in the murine myocardial infarction model in male Swiss mice (n = 7) by ligation of the left coronary artery. At day 7 after ligation, OG488-cNGR (0.75 mg/kg) or OG488 (0.31 mg/kg) was injected intravenously. The fluorescent intensity (Fl) was measured in the border zone and infarct area with fluorescence microscopy. FI peaked at 15 min after injection and decreased to 17.8% of the peak FI value at 12 h (residence half-life (t_1/2_), 9.1 h), and then to background level (2%) at 24 h. Administration of 20-fold excess cNGR 15 min after OG488-cNGR injection rapidly decreased FI in the infarct heart with the residence t_1/2_ of 1.3 h. No accumulation in normal myocardium was detected. OG488-cNGR and OG488 were rapidly cleared from the plasma by the kidney with the plasma t_1/2_ of 15 min and 7.7 min, respectively. No accumulation of OG488-cNGR was observed in the sham-operated heart (n = 3). OG488 alone exhibited little accumulation in the infarct heart (n = 3). Two-photon laser scanning microscopy experiments confirmed co-localization of OG488-cNGR with CD13/APN and the endothelial marker CD31 on the vessels in the border zone and infarct area of the infarct heart. CD13 mRNA expression was significantly up-regulated in the border zone and infarct area, but not in other areas of the infarcted heart and the sham operated hearts. CD13 mRNA expression in the border zone and infarct area peaked at 7 days after myocardial infarction with a significant increase of 10-20 folds, confirming that CD13 is induced in the murine myocardial infarction model.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EP-3533+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EP-3533+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EP-3533+human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Folkman J. (1995). Angiogenesis in cancer, vascular, rheumatoid and other disease. Nat Med.
4 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
5 Carmeliet P. (2004). Manipulating angiogenesis in medicine. J Intern Med.
6 Miller J.C., Pien H.H., Sahani D., Sorensen A.G., Thrall J.H. (2005). Imaging angiogenesis: applications and potential for drug development. J Natl Cancer Inst.
7 Riemann D., Kehlen A., Langner J. (1999). CD13--not just a marker in leukemia typing. Immunol Today.
8 Sato Y. (2004). Role of aminopeptidase in angiogenesis. Biol Pharm Bull.
9 Corti A., Curnis F., Arap W., Pasqualini R. (2008). The neovasculature homing motif NGR: more than meets the eye. Blood.
10 Curnis F., Arrigoni G., Sacchi A., Fischetti L., Arap W., Pasqualini R., Corti A. (2002). Differential binding of drugs containing the NGR motif to CD13 isoforms in tumor vessels, epithelia, and myeloid cells. Cancer Res.
11 Arap W., Pasqualini R., Ruoslahti E. (1998). Cancer treatment by targeted drug delivery to tumor vasculature in a mouse model. Science.
12 Buehler A., van Zandvoort M.A., Stelt B.J., Hackeng T.M., Schrans-Stassen B.H., Bennaghmouch A., Hofstra L., Cleutjens J.P., Duijvestijn A., Smeets M.B., de Kleijn D.P., Post M.J., de Muinck E.D. (2006). cNGR: a novel homing sequence for CD13/APN targeted molecular imaging of murine cardiac angiogenesis in vivo. Arterioscler Thromb Vasc Biol.
13 von Wallbrunn A., Waldeck J., Holtke C., Zuhlsdorf M., Mesters R., Heindel W., Schafers M., Bremer C. (2008). In vivo optical imaging of CD13/APN-expression in tumor xenografts. J Biomed Opt.